# ^68^Ga-Labeled β-aminoalanine, γ-aminohomoalanine, and ε-aminolysine conjugates of 1,4,7-triazacyclononane-1,4,7-triacetic acid

Chemical name: | ^68^Ga-labeled β-aminoalanine, γ-aminohomoalanine, and ε-aminolysine conjugates of 1,4,7-triazacyclononane-1,4,7-triacetic acid | [image]
Abbreviated name: | ^68^Ga-1a-c | [image]
Synonym: | ^68^Ga-1a, ^68^Ga-1b, ^68^Ga-1c | [image]
Agent Category: | Others (amino acid) | [image]
Target: | Amino acid transporters | [image]
Target Category: | Transporters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | Gallium-68 (^68^Ga) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of 1a-c (n = 1, β-aminoalanine; n = 2, γ-aminohomoalanine; and n = 4, ε-aminolysine) by Shetty et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=amino%20acid%20and%20imaging%20and%20amino%20acid%20transporters)]

The ^68^Ga-labeled β-aminoalanine, γ-aminohomoalanine, and ε-aminolysine conjugates of 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA), abbreviated as ^68^Ga-1a, ^68^Ga-1b, and ^68^Ga-1c, respectively, were synthesized by Shetty et al. for positron emission tomography (PET) of tumors (1).

Radiolabeled amino acids represent a diverse class of tracers that target the increased amino acid transport in cancer cells (2, 3). To date, >20 distinct amino acid transporters have been identified in mammalian cells, and these transporters differ in terms of substrate specificity, tissue expression patterns, sodium and other ion dependence, pH sensitivity, and transport mechanism (4, 5). Because of increased demand for amino acids in malignant cells, some transporters have been shown to be overexpressed in different types of tumors, and the process of amino acid transport is relatively fast (1, 2, 6). These features make tumor imaging with amino acid tracers possible within 20 min. Indeed, there is growing evidence that radiolabeled amino acids have the potential to overcome some of the limitations of 2-deoxy-2-[^18^F]fluoro-D-glucose ([^18^F]FDG) in tumor imaging, especially in the imaging of primary and recurrent brain tumors, neuroendocrine tumors, and prostate cancers (2, 3, 7). Different studies also showed that radiotracers that target different amino acid transporters exhibit different imaging properties that may provide unique biological information of tumors (1, 2, 8).

The first group of widely investigated amino acids is the analogs of phenylalanine and tyrosine (2, 3). Because of their bulky neutral side chains, these natural amino acids are the substrates of system L transporters and have been proven to be useful for tumor imaging, particularly for brain tumors. The limitation common to most of the natural amino acids is the susceptibility to in vivo metabolism, which decreases tumor specificity and complicates kinetic analysis. Because none of the natural amino acids contain fluorine or iodine, labeling with fluorine-18 or iodine-123 while retaining identical biological activity is also difficult. These shortcomings associated with natural amino acids can be partially overcome by using non-natural amino acids. Typically, non-natural amino acids are neither metabolized nor readily incorporated into protein in vivo (1-3). One group of non-natural amino acids is α,α-dialkyl amino acids, which are generated by substituting the α-carbon hydrogen of natural amino acids with a methyl group or other alkyl chains. These amino acids are primarily the substrates of system A transporters. The second group is alicyclic amino acids, which are α,α-dialkyl amino acids with side chains bonded covalently to each other to form a cyclic ring. These amino acids are the substrates of system L transporters. The third group is the non-natural proline derivatives, which exhibit different transport selectivity. One challenge in developing amino acid radiotracers is to overcome the low selectivity and the decreased recognition after radiolabeling to specific transporters (2, 3, 8). Another challenge is the low uptake of amino acid agents in tumors, which leads to less sensitivity for tumor detection than with [^18^F]FDG (7).

Shetty et al. synthesized a group of ^68^Ga-labeled alanine and lysine derivatives of NOTA, 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA), 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid (DO2A), and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid (DO3A) (1, 8). The four bifunctional chelating agents have similar sizes, but they differ in the net charges and stability because of the different numbers of pendent carboxylate arms. The amino acids have been conjugated to one of the carboxylate arms, and the nitrogen atoms in the heterocyclic ring are presumed to coordinate with metals to form chelates. Biodistribution studies and PET imaging indicate the structure–activity relationship of the amino acid derivatives, and the selective uptakes of these compounds by different cancer tissues might provide an insight on the different modes of amino acid uptake by cancer cells (1, 8).

This chapter summarizes the data obtained with ^68^Ga-labeled NOTA derivatives: ^68^Ga-1a (^68^Ga-NOTA-β-aminoalanine), ^68^Ga-1b (^68^Ga-NOTA-γ-aminohomoalanine), and ^68^Ga-1c (^68^Ga-NOTA-ε-aminolysine). These NOTA derivatives were comparatively analyzed with the corresponding DOTA derivatives (^68^Ga-2a, ^68^Ga-2b, and ^68^Ga-2c, respectively) (1).

### Related Resource Links:

Amino acid transporter-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amino+acid+transporter+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Amino acid transporter articles in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/?term=amino+acid+transporter)

Amino acid transporter related clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amino+acid+transporter)

Amino acid transporter related bioassays in PubChem BioAssay (http://www.ncbi.nlm.nih.gov/pcassay/?term=amino+acid+transporter)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20926300)]

The protected β-amino-L-alanine was synthesized from N-tert-butyl-L-serine methyl ester. Conjugation of NOTA with protected β-amino-L-alanine was performed in aqueous solution using 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide hydrochloride as a coupling reagent to obtain the alanine conjugate. Hydrolysis of the protected esters using LiOH, followed by hydrochloric acid, resulted in the formation of compound 1a (NOTA-β-aminoalanine) as a hydrochloride salt.

The γ-amino-L-homoalanine was purchased, and the ε-aminolysine was synthesized from N^α^-boc-N^ε^-benzyloxycarbonyl-lysine by tert-butyl esterification and subsequent deprotection. Conjugation of γ-amino-L-homoalanine and ε-aminolysine with NOTA was performed separately with N,N'-dicyclohexylcarbodiimide as a coupling agent and pyridine as a base. Further hydrolysis and deprotection resulted in the formation of compound 1b (NOTA-γ-aminohomoalanine) and compound 1c (NOTA-ε-aminolysine), respectively. All final products were purified. The structure of Ga-complexed NOTA-aminoalanine (1a) in aqueous solution was confirmed with multinuclear magnetic resonance spectroscopy (1).

The NOTA and DOTA derivatives were labeled with ^68^Ga either at room temperature or in a boiling water bath (1). The labeling efficiency was >95% for all agents, and no free ^68^Ga was found after purification. The specific activities of the purified agents were in the range 1.94–9.21 GBq/μmol (52.43–248.92 mCi/µmol). Stability studies at room temperature confirmed the stability of all agents for >4 h. The chelating agents, DOTA and NOTA, were also labeled with ^68^Ga as controls for the in vitro protein binding and cell uptake studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20926300)]

Shetty et al. performed protein binding studies by incubating the agents with human serum at 37°C for 10 min and 1 h, respectively (1). ^68^Ga-1b showed the lowest level of protein binding (1.71% at 10 min and 1.44% at 1 h), followed by ^68^Ga-1c (2.33% at 10 min and 2.64% at 1 h) and ^68^Ga-1a (3.07% at 10 min and 3.77% at 1 h).

In comparison with the corresponding DOTA derivatives, all NOTA derivatives had lower levels of serum protein binding. Of these, ^68^Ga-1b showed the lowest level of protein binding and ^68^Ga-2a showed the highest level of binding (9.87% at 10 min and 9.81% at 1 h). Only the DOTA derivatives showed significant increases in protein binding over time (1).

Cell uptake studies after incubation of the cells with each agent showed that all three agents had significantly higher uptakes than the control compounds (^68^Ga-NOTA and ^68^Ga-DOTA) in both Hep3B (a human hepatoma cell line) and CT-26 (a mouse colon cancer cell line) cells (1). Of the three agents, ^68^Ga-1a showed the highest uptake in both cell lines.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20926300)]

The biodistribution of ^68^Ga-1a, ^68^Ga-1b, and ^68^Ga-1c (10 μCi/0.1 ml (0.37 MBq/0.1 ml)) was investigated after tail vein injection in mice bearing human colon cancer CT-26 xenografts (n = 4 mice/time point for each agent) (1). Mice were euthanized at different times (10, 30, 60, and 120 min) after injection, and counts were obtained with a γ-scintillation counter. Tumor uptakes for all three agents were higher than those for most organs, except for the kidneys. Tumor/blood ratios were similar for the three agents up to 60 min after injection but differed at 120 min. The tumor/blood ratios for ^68^Ga-1a, ^68^Ga-1b, and ^68^Ga-1c were 4.36, 3.54, and 3.50, respectively, at 120 min after injection. Tumor/muscle ratios were different among the agents. The highest tumor/muscle ratio was achieved by ^68^Ga-1c (4.09), followed by ^68^Ga-1b (2.72) and ^68^Ga-1a (1.62) at 30 min after injection.

PET imaging in mice bearing human colon cancer CT-26 xenografts was performed at 30 min after injection of the agents (0.6–0.8 mCi (22.2–29.6 MBq)) through the tail vein. High levels of kidney and bladder activity were observed for all agents, indicating rapid renal excretion. Tumor uptakes were visualized by PET with all agents, but ^68^Ga-1b demonstrated the highest tumor/muscle ratio (12.3).

In comparison between DOTA and NOTA derivatives, all agents showed fast renal excretion and blood clearance, low nonspecific uptake in normal organs except for kidneys, and relatively high uptake in tumor tissues (1). In biodistribution studies, the tumor/blood ratios for NOTA-amino acid derivatives were higher than those for DOTA-amino acid derivatives at 2 h, although the ratios were similar for all six agents at 30 min after injection, which might be related to the higher serum protein binding by DOTA derivatives. In PET imaging, ^68^Ga-1b demonstrated the highest tumor/muscle ratio (12.3), followed by ^68^Ga-2a (5.9) and ^68^Ga-2b (4.3). These results suggest that ^68^Ga-1b is more favorable than others for use in PET imaging of tumors (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shetty D., Jeong J.M., Ju C.H., Kim Y.J., Lee J.Y., Lee Y.S., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis and evaluation of macrocyclic amino acid derivatives for tumor imaging by gallium-68 positron emission tomography. Bioorg Med Chem.
2 McConathy, J., W. Yu, N. Jarkas, W. Seo, D.M. Schuster, and M.M. Goodman, Radiohalogenated nonnatural amino acids as PET and SPECT tumor imaging agents. Med Res Rev, 2011
3 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
4 Ganapathy V., Thangaraju M., Prasad P.D. (2009). Nutrient transporters in cancer: relevance to Warburg hypothesis and beyond. Pharmacol Ther.
5 Goberdhan D.C. (2010). Intracellular amino acid sensing and mTORC1-regulated growth: new ways to block an old target?. Curr Opin Investig Drugs.
6 Fuchs B.C., Bode B.P. (2005). Amino acid transporters ASCT2 and LAT1 in cancer: partners in crime?. Semin Cancer Biol.
7 la Fougere C., Suchorska B., Bartenstein P., Kreth F.W., Tonn J.C. (2011). Molecular imaging of gliomas with PET: Opportunities and limitations. Neuro Oncol.
8 Shetty D., Jeong J.M., Ju C.H., Lee Y.S., Jeong S.Y., Choi J.Y., Yang B.Y., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis of novel 68Ga-labeled amino acid derivatives for positron emission tomography of cancer cells. Nucl Med Biol.